# ^99m^Tc-labeled ior-egf/r3 monoclonal antibody against epidermal growth factor receptor

Chemical name: | ^99m^Tc-labeled ior-egf/r3 monoclonal antibody against epidermal growth factor receptor
Abbreviated name: | ^99m^Tc-ior-egf/r3 MAb
Synonym:
Agent Category: | Monoclonal antibody
Target: | Epidermal growth factor receptor
Target Category: | Antibody-receptor binding
Method of detection: | Single photon emission computed tomography (SPECT); Gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | Not required
Studies: | - In vitro; - Rodents; - Humans | Click here for EGFR protein and nucleotide sequence (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_005228) information.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+ior+egf%2Fr3&WebEnv=0ItbmbiVqxQA99Xvgf1mZBgqdKFlYgdwXR2LUbyCmPZ5BM6Ah9CejwW9zAHnV5VGgLljy1GS2YeTkz%40255E7CA966D61D00_0011SID&WebEnvRq=1)]

Overexpression of the epidermal growth factor receptor (EGFR) is a characteristic feature of a variety of cancers such as breast, ovarian, lung, head and neck, bladder, and colon cancers (1). The EGFR is a 170-kDa transmembrane protein that promotes cell proliferation on binding of the autocrine epidermal growth factor (EGF) or the transforming growth factor α (TGFα). The EGFR operates through a receptor-associated tyrosine kinase–mediated signal transduction pathway. The progression of some cancers is attributed to both an increased level, and activation of EGFR by EGF and TGFα or to a constitutive activation of the tyrosine kinase pathway caused by the development of a mutated receptor kinase. In an effort to develop therapy against cancers that develop as a result of increased EGFR activity or a mutated receptor kinase, a variety of EGFR inhibitors have been developed that either compete with EGF and TGFα for receptor binding (e.g., monoclonal antibodies (MAb) that target the receptor) or are small molecules that inhibit activation of the receptor tyrosine kinase signaling pathway (2).

The murine MAb ior egf/r3, which binds to the external domain of the human EGFR, was generated at the Center of Molecular Immunology in Havana, Cuba (3), and has been shown to inhibit the EGF-dependent growth of various cell lines (4). This MAb was also labeled with metastable radioactive technetium (^99m^Tc) to obtain ^99m^Tc-ior-efg/r3 and evaluated in clinical trials for the treatment of patients with epithelial and advanced brain tumors (3, 5-8).

A freeze-dried kit formulation for direct labeling of ior-efg/r3 with ^99m^Tc has also been published (9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+ior-egf%2Fr3+synthesis&WebEnv=0gt_7qVHj3qkMdlNoBIVIBNAjNgWTRNWRJKjY-rAHbwClqLVtSt6f6gX_e4HF2eVh0SiM1bTF5H8FS%40255E7CA966D61D00_0011SID&WebEnvRq=1)]

The MAb ior-efg/r3 was secreted by a hybridoma produced by the fusion of mouse myeloma and splenocytes from Balb/c mice immunized with a partially purified fraction of the EGFR from human placenta as described by Fernandez et al. (10). Purification of ior-efg/r3 was not described by the investigators. The radiolabeling of ior-egf/r3 with ^99m^Tc has been detailed by Morales et al. (3) and is described briefly below.

The ior-efg/r3 MAb in phosphate-buffered saline (PBS) was reduced with a molar excess of mercaptoethanol at room temperature for 30 min. The reduced MAb was then purified with a Sephadex-G25M column and eluted in PBS. Integrity of the reduced MAb was compared to the native MAb by nonreducing polyacrylamide gel electrophoresis and size exclusion chromatography on a Superose 12 HR 10/30 column. Ellmans reagent and a micro method were used to determine the number of free sulphydryl groups in the reduced MAb (11, 12).

To radiolabel the reduced MAb, an aliquot of the reduced MAb was mixed with Medronate II bone agent methyl diphosphonate (MDP) kit reconstituted in saline. This solution was then mixed with 37 MBq (1 mCi) pertechnetate (^99m^TcO_4_^-^). Labeling efficiency of the reaction was determined by ascending paper chromatography, and radiocolloids were determined by cellulose nitrate electrophoresis. The labeling efficiency of the procedure was >98%. Specific activity of the product was not provided by the investigators.

Preparation of the freeze-dried kit formulation has been described by Morales et al. (9). For this, an aliquot of the reduced MAb was mixed with MDP containing 1% of mannitol, sorbitol, trehalose, glucose, sucrose, or inositol as lyoprotectants. The mixture was then frozen in liquid nitrogen. The frozen mixture was lyophilized for 24 h, vacuum-sealed, and stored at 4ºC until required. To label the freeze-dried formulation, the lyophilized MAb was mixed with ^99m^TcO_4_^-^ as described above. The labeling efficiency, determined as detailed above, was >97% only for the trehalose, glucose, sucrose, and inositol formulations. The labeling efficiency of formulations containing mannitol and sorbitol was <93% and contained approximately 7 to 8% ^99m^Tc-MDP as an impurity.

Unless otherwise specified, all of the animal and human studies described below appear to have been performed with the non–freeze-dried version of the ^99m^Tc-ior-egf/r3 formulation.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+labeled+egf%2Fr3+in+vitro&WebEnv=0cZyTMHifPnGLN-CPXSh3k1cfTs6-VHtRRMG_wbQoSGMqMT3G8bTrqcStqUd7mKSDc_6mIaqfsMIR%402640081266EA9960_0012SID&WebEnvRq=1)]

No publications are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+labeled+egf%2Fr3+rodentia&WebEnv=0XoCp_sXzZq2pZjhGiCP4Ndfp9P9laMDrbpH1F4-3luLxfJ6dBD1oDJI-bjRZyhf6oV-8eG4gY36_%402640081266EA9960_0012SID&WebEnvRq=1)]

The biodistribution of ^99m^Tc-ior-efg/r3 was studied in Balb/c mice (3). Radioactivity was observed in the blood, kidneys, heart, lungs, and large intestine of the animals at 4 h after administration. At 24 h after injection, a reduced amount of the label was detected in these organs.

Biodistribution of the freeze-dried formulation of the ^99m^Tc-ior-efg/r3 MAb was investigated in rats (9). The radioactivity accumulated primarily in the liver, kidneys, and lungs of these animals. The liver and lungs lost most of the label by 24 h after administration. The kidneys maintained almost a constant level of accumulated radioactivity in the time after the injection. Although no data was presented on the accumulation of radioactivity in the bladder, the investigators suggested that the accumulation of the label in the kidney indicated that the radiolabel was cleared from the animals primarily through the urinary bladder route.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+ior+efg%2Fr3+non-primate+mammals&WebEnv=01pbOW319R1kGIa-n6F4Zniqm1OzK-6rZP_-Ak2a5IDOaipyTJhJJfRRroEJSPV6tpAYyGhHjMIjGO%4025624DB566FF0130_0169SID&WebEnvRq=1)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+ior+efg%2Fr3+non-human+primates&WebEnv=0aaIdRucqeRGXm5soRKfNT2d7vwMIcAM2i7UuSaHuM_Xm7qbin09q8lBxs6O8Guj5EAyNE18A9jRnF%4025624DB566FF0130_0169SID&WebEnvRq=1)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+efg%2Fr3+Humans&WebEnv=0CDutU0Rueaxt21zMQFAzoAh5xslYjsVvHXsyqnJMVcRI0ll6BwA85Zy6ObsDCIEi0FEW-b8s1Ifg_%4025624DB566FF0130_0169SID&WebEnvRq=1)]

The biodistribution of ^99m^Tc-ior-egf/r3 was investigated with the use of immunoscintigraphy in patients with tumors of epithelial origin (7). Significant accumulation of the label was observed in the liver (~48% of total), heart (~3.5% of total), and spleen (~3.1% of total) at 5 min after the bolus infusion. At 24 h after infusion, the amount of radioactivity detected in these organs was significantly lower (liver, ~3.2%; heart, ~0.1%; spleen, ~0.06%). The tumor and liver uptake as well as plasma clearance kinetics of radioactivity in the patients were also monitored during this study. An accumulation of radioactivity was observed in the tumors and liver up to 5 h after injection. The liver subsequently showed a steady loss of radioactivity up to 24 h. During the same period a steady loss of label was observed in the plasma. The tumors showed an increase in label accumulation up to 5 h followed by a steady amount of radioactivity up to 24 h after administration of the labeled MAb.

In another study from the same laboratory, the pharmacokinetics and clearance of the labeled antibody were investigated in patients with tumors of epithelial origin (13). With results obtained from this investigation it was concluded the labeled MAb had an elimination half-life of ~21 h. An analysis of the urine samples from these patients showed that clearance of radioactivity through this route was only ~5% of the injected dose at 24 h after administration, and a fast protein liquid chromatography analysis showed little decomposition (i.e., only 6–7%) of the labeled MAb to smaller molecular weight species of the molecule.

The clinical trial safety and diagnostic efficacy of ^99m^Tc-ior-egf/r3 was also investigated in patients with tumors of epithelial origin (8). The overall sensitivity, specificity, accuracy, and positive and negative predictive values for the immunoscintigraphic images were 84.2%, 100%, 86.5%, 100%, and 52.4%, respectively. From this study it was concluded immunoscintigraphy with ^99m^Tc-ior-egf/r3 could be used for the diagnosis and follow-up of patients with tumors of epithelial origin.

## References

1 Gullick W.J. (1991). Prevalence of aberrant expression of the epidermal growth factor receptor in human cancers. Br Med Bull.
2 Dancey J.E. (2003). Recent advances of molecular targeted agents: opportunities for imaging. Cancer Biol Ther.
3 Morales A.A., Crespo F.Z., Gandolff G.N., Iznaga Escobar N., Perez N.P., Hernandez J.C. (1998). Technetium-99m direct radiolabeling of monoclonal antibody ior egf/r3. Nucl Med Biol.
4 Suarez Pestana E., Greiser U., Sanchez B., Fernandez L.E., Lage A., Perez R., Bohmer F.D. (1997). Growth inhibition of human lung adenocarcinoma cells by antibodies against epidermal growth factor receptor and by ganglioside GM3: involvement of receptor-directed protein tyrosine phosphatase(s). Br J Cancer.
5 Crombet T., Torres O., Neninger E., Catala M., Rodriguez N., Ramos M., Fernandez E., Iznaga N., Perez R., Lage A. (2001). Phase I clinical evaluation of a neutralizing monoclonal antibody against epidermal growth factor receptor. Cancer Biother Radiopharm.
6 Crombet T., Torres O., Rodriguez V., Menendez A., Stevenson A., Ramos M., Torres F., Figueredo R., Veitia I., Iznaga N., Perez R., Lage A. (2001). Phase I clinical evaluation of a neutralizing monoclonal antibody against epidermal growth factor receptor in advanced brain tumor patients: preliminary study. Hybridoma.
7 Iznaga-Escobar N., Torres L.A., Morales A., Ramos M., Alvarez I., Perez N., Fraxedas R., Rodriguez O., Rodriguez N., Perez R., Lage A., Stabin M.G. (1998). Technetium-99m-labeled anti-EGF-receptor antibody in patients with tumor of epithelial origin: I. Biodistribution and dosimetry for radioimmunotherapy. J Nucl Med.
8 Ramos-Suzarte M., Rodriguez N., Oliva J.P., Iznaga-Escobar N., Perera A., Morales A., Gonzalez N., Cordero M., Torres L., Pimentel G., Borron M., Gonzalez J., Torres O., Rodriguez T., Perez R. (1999). 99mTc-labeled antihuman epidermal growth factor receptor antibody in patients with tumors of epithelial origin: Part III. Clinical trials safety and diagnostic efficacy. J Nucl Med.
9 Morales A.A., Nunez-Gandolff G., Perez N.P., Veliz B.C., Caballero-Torres I., Duconge J., Fernandez E., Crespo F.Z., Veloso A., Iznaga-Escobar N. (1999). Freeze-dried formulation for direct 99mTc-labeling ior-egf/r3 MAb: additives, biodistribution, and stability. Nucl Med Biol.
10 Fernandez A., Spitzer E., Perez R., Boehmer F.D., Eckert K., Zschiesche W., Grosse R. (1992). A new monoclonal antibody for detection of EGF-receptors in western blots and paraffin-embedded tissue sections. J Cell Biochem.
11 Ellman G.L. (1959). Tissue sulfhydryl groups. Arch Biochem Biophys.
12 Escobar N.I., Morales A., Nunez-Gandolff G. (1996). Micromethod for quantification of SH groups generated after reduction of monoclonal antibodies. Nucl Med Biol.
13 Iznaga-Escobar N., Torres Arocha L.A., Morales Morales A., Ramos Suzarte M., Rodriguez Mesa N., Perez Rodriguez R. (1998). Technetium-99m-antiepidermal growth factor-receptor antibody in patients with tumors of epithelial origin: part II. Pharmacokinetics and clearances. J Nucl Med.